# ^64^Cu-Labeled PEGylated nano-graphene oxide (GO) covalently linked to NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody TRC105

Chemical name: | ^64^Cu-Labeled PEGylated nano-graphene oxide (GO) covalently linked to NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody TRC105
Abbreviated name: | [^64^Cu]-NOTA-GO-TRC105
Synonym:
Agent Category: | Antibody
Target: | CD105 (endoglin) antigen
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD105&cmd=DetailsSearch)]

The CD105 antigen (endoglin) is a hypoxia-inducible, 180-kDa, disulfide-linked, homodimeric transmembrane glycoprotein that is a co-receptor for the transforming growth factor β (TGF-β) (1). Both CD105 and TGF-β are expressed at low levels in resting endothelial cells, but they are overexpressed in cancerous lesions and play a significantly proangiogenic role in remodeling the vasculature of malignant tumors (2). It has been shown that the levels of CD105 in endothelial tissues correlate well with the degree of cell proliferation and that the antigen is a suitable biomarker to quantify tumor angiogenesis and can be used to determine the prognostic outcome for cancer patients (3). The biological activity of CD105 has been discussed in detail by Seon et al. (4). Investigators have demonstrated that immunotoxins and radioimmunoconjugates generated with anti-CD105 monoclonal antibodies (mAbs) can inhibit angiogenesis and prevent the growth and metastasis of cancerous tumors (4). For translation to the clinic, a human/mouse chimeric anti-CD105 mAb (designated c-SNj6 or TRC105) was generated, and shown to have suitable pharmacokinetic, toxicological, and immunogenicity characteristics for use in non-human primates (5). Currently, a clinical trial (http://clinicaltrials.gov/ct2/show/NCT01326481?term=endoglin&rank=5) is in progress to evaluate the use of TRC105 for the treatment of metastatic breast cancer.

TRC105 has been labeled with ^64^Cu (6) and ^89^Zr (7), respectively, and has been reported to detect the expression of CD105 with positron emission tomography (PET) imaging in xenograft tumors in mice. In another study, TRC105 was conjugated to IRDye 800CW, a near-infrared fluorescent (NIRF) dye, and the expression of CD105 in tumors was visualized with NIRF imaging (8). TRC105 has also been conjugated with ^64^Cu and IRDye 800CW to develop a dual-modality (PET/NIRF) imaging agent that can be used to detect murine breast cancer 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors in mice (9). Recently, TRC105 was conjugated to 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA) and labeled with ^66^Ga, and the radioimmunoconjugate was shown to be suitable for the visualization of CD105 expression with PET in 4T1 cell xenograft tumors in mice (10).

Investigators have recently become interested in the use of PEGylated graphene oxide (GO; to read about the physical and chemical properties of graphene, see Feng and Liu (11)), a carbon-based material, in biomedical applications such as drug delivery (12), cancer therapy (13), and preclinical in vivo imaging and ablation of tumors in mice (14). In a proof-of-principle study, Hong et al. (15) used PET to evaluate ^66^Ga-labeled NOTA covalently linked to a sheet of PEGylated nano-GO conjugated to TRC105 (NOTA-GO-TRC105) for the biodistribution and visualization of xenograft tumors that express the CD105 antigen in mice. In a similar study with a different tumor model the biodistribution and efficacy of ^64^Cu-labeled NOTA-GO-TRC105 ([^64^Cu]-NOTA-GO-TRC105) to detect xenograft tumors that expressed the CD105 in mice was investigated with PET (16).

### Related Resource Links

TRC105 (http://www.ncbi.nlm.nih.gov/books/?term=TRC105+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Other anti-CD105 antibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-CD105+antibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD105 (endoglin) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/BC014271.2) sequences

CD105 gene information (http://www.ncbi.nlm.nih.gov/gene/2022) (Gene ID: 2022)

CD105 in Online Mendelian Inheritance in Man Database (http://omim.org/entry/131195) (OMIM)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=TRC105) related to TRC105

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-GO-TRC105%20synthesis&cmd=DetailsSearch)]

The covalent linking of NOTA to PEGylated GO (NOTA-GO) and the synthesis of NOTA-GO-TRC105 for radiolabeling with ^64^Cu for in vivo PET imaging and biodistribution studies is described elsewhere (16). Fluorescein isothiocyanate (FITC)-labeled GO (FITC-GO) and FITC-GO-TRC105 were synthesized to investigate the in vitro binding affinity and specificity of the complexes for CD105 with fluorescence techniques (16). The average number of NOTA molecules covalently linked to a sheet of GO was not reported. The average small sheet size range of NOTA-GO and NOTA-GO-TRC105 was 10–50 nm as determined with atomic force microscopy (16). The average diameters of the two GO conjugates were 21.9 ± 0.6 nm and 27.0 ± 0.9 nm, respectively, as determined with dynamic light scattering measurements (16). The zeta-potentials of NOTA-GO and NOTA-GO-TRC105 were determined to be −9.46 ± 4.74 mV and 0.08 ± 5.35 mV, respectively (16).

NOTA-GO and NOTA-GO-TRC105 were respectively labeled with ^64^Cu, and the radiolabeled products were purified on PD-10 columns with phosphate-buffered saline (pH not reported) as the mobile phase (16). The preparation and purification procedures for [^64^Cu]-NOTA-GO or [^64^Cu]-NOTA-GO-TRC105 were completed in 90 ± 10 min (n = 10 preparations). The radiochemical yields, radiochemical purities, and specific activities of both [^64^Cu]-NOTA-GO and [^64^Cu]-NOTA-GO-TRC105 were reported to be 76 ± 8% (based on 30 μg NOTA-GO or NOTA-GO-TRC105), >95%, and ~0.9 GBq/mg (24.3 mCi/mg), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-GO-TRC105%20in%20vitro&cmd=DetailsSearch)]

The stability of [^64^Cu]-NOTA-GO and [^64^Cu]-NOTA-GO-TRC105 was investigated by incubating the respective tracers in complete mouse serum at 37°C for up to 48 h, and the incubation mixtures were sampled at various time points to determine the percentage of radioactivity retained on the GO conjugates (16). Both ^64^Cu-labeled GO conjugates were reported to retain >90% of the radioactivity at all the time points as determined with filtration through a 100-kDa cutoff filtration device. This study indicated that the two radiolabeled complexes would have excellent stability under in vivo conditions.

Flow cytometric analysis of HUVEC (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1730&Template=cellBiology) cells (human umbilical vein endothelial cells that have a high expression of CD105) exposed to 50 μg/mL FITC-GO-TRC105 (based on GO content) showed that the cells had >570-fold higher fluorescence intensity compared with the untreated cells (16). Treatment of HUVEC cells with FITC-GO or TRC105 alone enhanced the fluorescence only by ~6-fold. Cells blocked with 3.33 nmol TRC105 and then treated with FITC-GO-TRC105 as above had ~100-fold lower fluorescence intensity compared with cells exposed to FITC-GO-TRC105 alone. This indicated that FITC-GO-TRC105 bound specifically to the CD105 antigen on the surface of the HUVEC cells. Minimal fluorescence was observed in MCF-7 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-22&Template=cellBiology) cells (a human breast cancer epithelial cell line that does not express the CD105; used as a negative control in this study), indicating that FITC-GO-TRC105 exhibited low non-specific binding to the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-GO-TRC105%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]-NOTA-GO and [^64^Cu]-NOTA-GO-TRC105 was investigated in mice bearing murine breast cancer 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors as described by Hong at al (16). The animals (n = 4 mice/group) were injected with the tracer (5–10 MBq (135–270 μCi) in each mouse) through the tail vein and euthanized at 3 h and 48 h postinjection (p.i.). All the major organs, including the tumors, were retrieved from the animals to determine the amount of radioactivity accumulated in the various tissues. Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). With both radiolabeled GO conjugates, the label was detected at 3 h p.i. mainly in the liver (~17.5% ID/g), followed by blood (~10.0% ID/g and ~15% ID/g for [^64^Cu]-NOTA-GO-TRC105 and [^64^Cu]-NOTA-GO, respectively), and spleen (~10% ID/g for both [^64^Cu]-NOTA-GO-TRC105 and [^64^Cu]-NOTA-GO). Tumors of mice injected with [^64^Cu]-NOTA-GO-TRC105 showed a significantly higher uptake of label (~6.0% ID/g; P < 0.05) compared with the amount detected in the lesions of mice injected with [^64^Cu]-NOTA-GO (~2.0% ID/g). All other organs showed a radioactivity uptake of <2.5% ID/g with both the tracers at all the time points. By 48 h p.i., the uptake of radioactivity from both tracers was similar in the blood (~2.5% ID/g), liver (~12.5% ID/g), spleen (~10% ID/g), and the tumors (~2.5% ID/g). Another group of mice (n = 4 animals) given a blocking dose of NOTA-GO-TRC105 (33.33 nmol/kg body weight) 2 h before administration of the radiolabeled GO immunoconjugate were euthanized at 48 h p.i. The accumulation of radioactivity in the blood, liver, spleen, and tumors of these animals was comparable to the uptake observed at 48 h p.i. in the normal tissues and lesions of animals injected with [^64^Cu]-NOTA-GO-TRC105 alone (16). The insignificant difference in the uptake of radioactivity between the tumors of the “blocked” animals and the lesions of animals injected with [^64^Cu]-NOTA-GO-TRC105 alone was attributed to clearance of the label from the tissues due to metabolism and degradation of the conjugate (16).

For PET imaging of mice bearing 4T1 cell tumors (n = 4 animals), the rodents were injected with 5–10 MBq (135–270 μCi) [^64^Cu]-NOTA-GO-TRC105 or [^64^Cu]-NOTA-GO through the tail vein, and static whole-body images of the animals were acquired at 0.5 h, 3 h, 16 h, 24 h, and 48 h p.i (16). Quantitative data for the various organs and the tumors were obtained from the images with region-of-interest analysis as described by Hong et al. (16). The amount of tracer in the blood was 9.7 ± 1.3% ID/g, 6.6 ± 0.5% ID/g, 4.4 ± 0.5% ID/g, 4.3 ± 0.2% ID/g, and 3.9 ± 0.1% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively, and the amount of label in the liver was 18.6 ± 1.3% ID/g, 14.1 ± 2.1% ID/g, 12.4 ± 1.9% ID/g, 13.2 ± 1.2% ID/g, and 13.7 ± 1.3% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively. The tumors were clearly visible at 0.5 h p.i. and showed a relatively stable uptake of radioactivity at all the time points (5.8 ± 0.6% ID/g, 5.3 ± 0.6% ID/g, 4.5 ± 0.6% ID/g, 4.0 ± 0.4% ID/g, and 3.4 ± 0.1% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively). At all the time points, the accumulation of radioactivity from [^64^Cu]-NOTA-GO-TRC105 in the muscles was reported to be <0.5% ID/g. In general, with [^64^Cu]-NOTA-GO the level and pattern of radioactivity uptake in the liver and blood was similar to that observed with [^64^Cu]-NOTA-GO-TRC105. With [^64^Cu]-NOTA-GO, the accumulation of the tracer in the tumors was 2.0 ± 0.3% ID/g, 2.1 ± 0.4% ID/g, 1.9 ± 0.4% ID/g, 2.2 ± 0.4% ID/g, and 2.4 ± 0.3% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively, but the uptake in the lesions was significantly lower than that observed with [^64^Cu]-NOTA-GO-TRC105 (P < 0.05) at all these time points.

To determine the in vivo target-binding specificity of [^64^Cu]-NOTA-GO-TRC105, the animals (n = 4 mice) were injected with 13.3 nmol nonradioactive TRC105 2 h before administration of the ^64^Cu-labeled GO immunoconjugate (16). PET images of the animals were acquired as before. The uptake of label in the tumors was calculated to be 2.0 ± 0.5% ID/g, 2.1 ± 0.3% ID/g, 2.6 ± 0.4% ID/g, 2.7 ± 0.3% ID/g, and 2.8 ± 0.2% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively, which was significantly lower (P < 0.05 at all the time points) than the accumulation observed in the lesions of animals injected with [^64^Cu]-NOTA-GO-TRC105 alone (for uptake values, see above). The amount of radioactivity detected in the liver and blood of animals given the blocking dose was similar to that of animals injected with [^64^Cu]-NOTA-GO-TRC105 alone at all the time points (the amount of radioactivity in the liver was 15.3 ± 2.0% ID/g, 14.6 ± 2.1% ID/g, 12.5 ± 1.7% ID/g, 11.9 ± 1.3% ID/g, and 11.4 ± 1.3% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively, and in the blood it was 10.2 ± 1.3% ID/g, 6.9 ± 0.9% ID/g, 5.3 ± 0.5% ID/g, 4.8 ± 0.2% ID/g, and 2.9 ± 0.1% ID/g at 0.5, 3, 16, 24, and 48 h p.i., respectively). Therefore, this study confirmed the in vivo binding specificity of the GO-radioimmunoconjugate to the CD105 antigen (16).

To confirm the uptake of NOTA-GO-TRC105 in CD105-specific tissues of mice bearing 4T1 cell tumors, the animals (n = 3 mice) were injected with 5 mg/kg body weight of the non-radiolabeled GO-immunoconjugate and euthanized at 3 h p.i (16). The tumors, liver, spleen, and muscles of the rodents were harvested, frozen, and cryo-sectioned for histological examination. Light microscopy revealed that high levels of NOTA-GO-TRC105 were present (seen as dark spots) only in tissue sections of the tumors, liver, and spleen, but not in the muscles of these animals. However, NOTA-GO was observed only in the sections of liver and spleen tissues obtained from animals injected with this GO-chelating agent complex. This study demonstrated that NOTA-GO-TRC105 specifically targets the CD105 antigen in the tumor. Immunofluorescence staining of the tissue slices for CD31 (a biomarker for the vasculature), with anti-mouse CD31 as the primary antibody and for CD105 using the TRC105 within NOTA-GO-TRC105 as the primary antibody, showed that the uptake of NOTA-GO-TRC105 in the liver and spleen was due to the non-specific capture of the complex by the reticuloendothelial system and not due to the specific targeting of CD105 on the vasculature. Almost no uptake of NOTA-GO-TRC105 was observed in the muscles and other normal tissues of the animals (16).

From these studies, the investigators concluded that [^64^Cu]-NOTA-TRC105 is a suitable agent to detect tumors that express the CD105 antigen in rodents (15).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-GO-TRC105%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-GO-TRC105%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-GO-TRC105%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

This work was supported in part by a grant from the National Institutes of Health through the UW Radiological Sciences Training Program 5 T32 CA009206-32.

## References

1 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
2 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
3 Fonsatti E., Nicolay H.J., Altomonte M., Covre A., Maio M. (2010). Targeting cancer vasculature via endoglin/CD105: a novel antibody-based diagnostic and therapeutic strategy in solid tumours. Cardiovasc Res.
4 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
5 Shiozaki K., Harada N., Greco W.R., Haba A., Uneda S., Tsai H., Seon B.K. (2006). Antiangiogenic chimeric anti-endoglin (CD105) antibody: pharmacokinetics and immunogenicity in nonhuman primates and effects of doxorubicin. Cancer Immunol Immunother.
6 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
7 Hong H., Severin G.W., Yang Y., Engle J.W., Zhang Y., Barnhart T.E., Liu G., Leigh B.R., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of CD105 expression with 89Zr-Df-TRC105. Eur J Nucl Med Mol Imaging.
8 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
9 Zhang Y., Hong H., Engle J.W., Yang Y., Theuer C.P., Barnhart T.E., Cai W. (2012). Positron Emission Tomography and Optical Imaging of Tumor CD105 Expression with a Dual-Labeled Monoclonal Antibody. Mol Pharm.
10 Engle J.W., Hong H., Zhang Y., Valdovinos H.F., Myklejord D.V., Barnhart T.E., Theuer C.P., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of tumor angiogenesis with a (66)ga-labeled monoclonal antibody. Mol Pharm.
11 Feng L., Liu Z. (2011). Graphene in biomedicine: opportunities and challenges. Nanomedicine (Lond).
12 Yang K., Wan J., Zhang S., Zhang Y., Lee S.T., Liu Z. (2011). In vivo pharmacokinetics, long-term biodistribution, and toxicology of PEGylated graphene in mice. ACS Nano.
13 Yang K., Zhang S., Zhang G., Sun X., Lee S.T., Liu Z. (2010). Graphene in mice: ultrahigh in vivo tumor uptake and efficient photothermal therapy. Nano Lett.
14 Zhang W., Guo Z., Huang D., Liu Z., Guo X., Zhong H. (2011). Synergistic effect of chemo-photothermal therapy using PEGylated graphene oxide. Biomaterials.
15 Hong H., Zhang Y., Engle J.W., Nayak T.R., Theuer C.P., Nickles R.J., Barnhart T.E., Cai W. (2012). In vivo targeting and positron emission tomography imaging of tumor vasculature with (66)Ga-labeled nano-graphene. Biomaterials.
16 Hong H., Yang K., Zhang Y., Engle J.W., Feng L., Yang Y., Nayak T.R., Goel S., Bean J., Theuer C.P., Barnhart T.E., Liu Z., Cai W. (2012). In vivo targeting and imaging of tumor vasculature with radiolabeled, antibody-conjugated nanographene. ACS Nano.